# ^125^I-Labeled chimeric monoclonal antibody, ch806, targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)

Chemical name: | ^125^I-Labeled chimeric monoclonal antibody, ch806, targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Abbreviated name: | [^125^I]-ch806
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, and functioning of the different members of the transmembrane epidermal growth factor receptor (EGFR) family are described elsewhere (1-3). The EGFR receptors are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signal transduction pathway, and they are overexpressed in many malignant epithelial tumors (1, 2). Overexpression of the EGFR in tumors has been attributed to gene amplification, and this phenomenon is believed to introduce mutations in the receptor (2, 4). Also, overexpression of the EGFR usually indicates a poor clinical prognosis for the patient (4). The most common mutation observed in the EGFR receptor is the deletion of a segment of the extracellular domain, including the ligand-binding region, which results in the generation of a variant known as the de2-7 EGFR or EGFRvIII (2, 4). The generation, structure, functions, and role of the EGFRvIII in tumor malignancy have been reviewed by Gan et al. (5). Although the EGFRvIII is nonresponsive to the ligand, it is constitutively active with a constantly operating downstream TK signaling pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastomas and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain the cancerous state of cells, several antibodies that inhibit the receptor activity and small molecules that block the downstream TK signaling pathway have been developed and have been approved by the United States Food and Drug Administration (FDA) for the treatment of certain cancers (2). The antibodies are directed toward the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which ultimately results in downregulation of the EGFR on the cell surface. However, because the EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). As a consequence, the monoclonal antibody (mAb) 806, which specifically targets the EGFRvIII, was generated and characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated as ch806, was developed (9) and evaluated in a phase I clinical trial with patients having cancerous tumors overexpressing the EGFRvIII (4). Results obtained from this trial indicated that ch806 could be a good biotherapeutic agent for the treatment of cancers expressing the ch806 antigen (4). In addition, several other clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) approved by the FDA are in progress to evaluate the targeting of EGFRvIII as a treatment against various cancers.

The internalization, intracellular trafficking, and biodistribution (in nude mice bearing xenograft human epidermoid carcinoma cell tumors) of mAb806 labeled with ^125^I and ^111^In, respectively, have been investigated by Perera et al. (8) and are described separately in MICAD (www.micad.nih.gov) (10, 11). The characterization and biodistribution (in nude mice bearing xenograft human glioblastoma cell tumors) of ch806 labeled with ^125^I ([^125^I]-ch806) or ^111^In ([^111^In]-ch806) have been investigated by Panousis et al. (9). The use of ^124^I-labeled ch806 for the detection of EGFRvIII-expressing xenograft human glioblastoma tumors in nude mice with an immuno–positron emission tomography (PET) technique was investigated by Lee et al. (6) and is described in another chapter in MICAD (12). This chapter describes the studies performed with [^125^I]-ch806. Studies performed with [^111^In]-ch806 are described separately in MICAD (13).

### Other sources of information

Human EGFR Gene (http://www.ncbi.nlm.nih.gov/gene/1956) (Gene ID: 1956)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200131&source=NATURE&output-format=graphic&ppage=1&genes_a=1956) (NCI-Nature Pathways Interactive Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-ch806%20synthesis&cmd=DetailsSearch)]

The production and ^125^I labeling of ch806 to obtain [^125^I]-ch806 was done using a modified chloramine-T method and is described elsewhere (9). The radiochemical purity of the [^125^I]-chAb was reported to be >98.6% as determined with instant thin-layer chromatography. The specific activity of [^125^I]-ch806 was reported to be ~0.040 MBq/6.6 pmol (~166.7 Ci/mmol). The final formulation and storage conditions of the radiolabeled chAb were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-ch806%20in%20vitro&cmd=DetailsSearch)]

The stability of [^125^I]-ch806 was determined in healthy human donor serum at 37°C and was reported to maintain a radiochemical purity of 95% for up to 7 days (9). Under the same storage conditions and duration, immunoreactivity of the labeled chAb with U87MG.de2-7 cells (a human glioma cell line generated to overexpress the EGFRvIII) was determined to be >65%. Using various cell lines expressing or overexpressing the EGFRvIII or the wild-type EGFR, respectively, it was shown that ch806 and the parental mAb806 had a similar receptor-binding profile.

The receptor association constant for [^125^I]-ch806 was reported to be 1.90 × 10^9^ M^-1^ compared with 1.1 × 10^9^ M^-1^ for the parental mAb806 as determined with the Lindmo assay using U87MG.de2-7 cells (9). The number of [^125^I]-ch806 molecules bound per cell was reported to be 4.7 × 10^5^ compared with 6.0 × 10^5^ for [^111^In]-ch806 (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-ch806%20rodentia&cmd=DetailsSearch)]

The biodistribution patterns of [^125^I]-ch806 and [^111^In]-chb806 were studied in BALB/c nude mice respectively bearing xenograft U87MB.de2-7 and A431 cell tumors (of human epidermoid carcinoma origin; overexpress the EGFR and do not express the EGFR, respectively) (9). Nude mice bearing FaDu xenograft tumors (of human squamous cell carcinoma origin) were used as controls for this study. The animals (n = 3–5 animals/time point) were injected with the respectively labeled chAb through the tail vein and euthanized at predetermined time points ranging from 4 h to 312 h post-injection (p.i.) for the collection of tumors and all major organs (9). All data of radioactivity accumulated in the various organs were presented as percent of injected dose per gram tissue (% ID/g). In general, the uptake and retention of label by the tumors was significantly (P < 0.001) lower at all time points with [^125^I]-ch806 (peaking at ~7.0% ID/g at 24 h) than with [^111^In]-chAb806 (peaking at ~31.0% ID/g at 48 h). With [^125^I]-ch806, the accumulation of radioactivity in the xenografts from 72 h to 168 h p.i. was more than six times lower than the uptake with [^111^In]-ch806 in the same period (9). During the entire study period, the accumulation of radioactivity from [^125^I]-ch806 and [^111^In]-ch806 in all major organs was ~10.0% ID/g, except for the kidneys and blood. The accumulation of radioactivity in these organs correlated to the level of tracer present in the blood pool of the animals. Lower uptake of the label and similar tracer biodistribution patterns were observed in all of the tissues from animals bearing the A431 or the FaDu xenograft tumors. No blocking studies using unlabeled ch806, mAb806, or another suitable anti-EGFR mAb were reported.

The half-life times of [^125^I]-ch806 and [^111^In]-chAb806 were determined to be 2.85 ± 0.24 h and 3.42 ± 0.92 h, respectively, using serum samples obtained from the tracer-injected animals (9). The total serum clearance for [^125^I]-ch806 was reported to be 0.063 ± 0.0003 ml/h; total serum clearance for [^111^In]-chAb806 was 0.045 ± 0.005 ml/h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-ch806%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-ch806%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=125I-ch806%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
2 Pines G., Kostler W.J., Yarden Y. Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Hasselbalch, B., U. Lassen, H.S. Poulsen, and M.T. Stockhausen, Cetuximab Insufficiently Inhibits Glioma Cell Growth Due to Persistent EGFR Downstream Signaling. Cancer Invest.
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Panousis C., Rayzman V.M., Johns T.G., Renner C., Liu Z., Cartwright G., Lee F.T., Wang D., Gan H., Cao D., Kypridis A., Smyth F.E., Brechbiel M.W., Burgess A.W., Old L.J., Scott A.M. (2005). Engineering and characterisation of chimeric monoclonal antibody 806 (ch806) for targeted immunotherapy of tumours expressing de2-7 EGFR or amplified EGFR. Br J Cancer.
10 Chopra, A., [125I]-Labeled monoclonal antibody 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., [111In]-Labeled CHX-A"-DTPA conjugated monoclonal antibody 806 (mAb 806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., [124I]-Labeled residulizing ligand IMP-R4 conjugated chimeric monoclonal antibody ch806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., [111In]-Labeled CHX-A"-DTPA conjugated chimeric antibody 806 (ch806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.